# [^123^I]-β-Methyl iodophenyl-pentadecanoic acid

Chemical name: | [^123^I]-β-Methyl iodophenyl-pentadecanoic acid
Abbreviated name: | [^123^I]-BMIPP
Synonym: | 15-(p-[^123^I]iodophenyl)-3(R,S)-methylpentadecanoic acid; [^125^I]-3(R,S)-BMIPP
Agent Category: | Compound
Target: | Myocardial tissue fatty acid metabolism
Target Category: | Uptake
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of Signal/Contrast: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+BMIPP)]

Under normal conditions the myocardium can metabolize several different types of substrates for energy. Although fatty acids supply almost 66% of the energy requirements of this tissue, the myocardium can also metabolize glucose (the second most preferred substrate), lactate, amino acids, and ketone bodies (1). Either through β-oxidation or glycolysis the fatty acids and glucose are, respectively, broken down to acetyl-coenzyme A (CoA), which is further oxidized through the tricarboxylic acid cycle to produce energy. Certain pathological conditions, such as ischemia, are known to alter myocardial metabolism, and the reduced availability of oxygen shifts the myocardium into an anaerobic mode that leads to an increased utilization of glucose for energy because glycolysis requires less oxygen in comparison to β-oxidation (2). Therefore, different imaging agents are used to assess myocardial changes observed during heart disease. For example, radioactive fluorodeoxyglucose ([^18^F]-FDG) is often used to evaluate glucose metabolism, labeled acetate is used to assess oxygen consumption, and fatty acids labeled with iodine (^123^I) are used for single-photon emission computed tomography (SPECT) of the heart (1).

Among the fatty acids, [^123^I]-β-methyl iodophenyl-pentadecanoic acid ([^123^I]-BMIPP), used as a racemic mixture ([^125^I]-3(R,S)-BMIPP), is used most frequently for SPECT imaging of the heart because the methyl group at the β position of the molecule slows β-oxidation of the fatty acid, which results in prolonged retention and improved quantitative imaging of the organ (3). Animal and clinical studies have shown that the CD36 molecule on the cell membrane plays an important role in the transport of BMIPP into the cell (4). It is then converted to BMIPP-CoA and rapidly incorporated into triglycerides (5). Using a dual mixture of [^125^I]-3(R)-BMIPP and [^131^I]-3(S)-BMIPP as surrogate molecules for [^123^I]-BMIPP to study the effect of BMIPP molecular configuration on its uptake and metabolism in the rat myocardium, it was shown that uptake of the 3(R)-BMIPP isomer was higher compared to 3(S)-BMIPP but the two isomers were metabolized in the same manner in the rat myocardium (6, 7). Morishita et al. proved that BMIPP was metabolized in the mitochondria of the tissue (8). Other investigators studying the metabolism of branched-chain fatty acids in the myocardium of rats with streptozotocin-induced acute or chronic diabetes mellitus concluded that the uptake of BMIPP was reduced in rats with chronic diabetes mellitus because the mitochondrial function was not normal in the myocardium of these animals (9).

In humans, [^123^I]-BMIPP was shown to be a superior cardiac SPECT imaging agent compared to its dimethyl analog, and it has been used extensively for this purpose in Japan and Europe (1, 7, 10). Akashi et al. investigated the significance of [^123^I]-BMIPP imaging in cardiac patients and concluded that this radiochemical enhanced the assessment of fatty acid metabolism disorders in the myocardium both under normal and diseased conditions (11). Nishimura and colleagues have shown that [^123^I]-BMIPP scintigraphy can be used to detect asymptomatic coronary artery disease and predict cardiac death and coronary artery stenosis in hemodialysis patients (12-14). In the United States, [^123^I]-BMIPP has been used for the imaging of ischemic heart and coronary artery disease as well as acute coronary syndrome in clinical trials (http://clinicaltrials.gov/ct2/results?term=123I+BMIpp) approved by the U.S. Food and Drug Administration. The use of [^123^I]-BMIPP for diagnostic imaging has been patented in the United States (15).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+BMIPP+synthesis)]

The synthesis of BMIPP has been described by Goodmen et al. (16). Briefly, a mixture of 3-methylglutaric anhydride and methanol was stirred at 100°C for 90 min, and the resulting clear, viscous oil (crude half-ester) was vacuum-distilled at 30°C for 30 min. The crude half-ester was then mixed with thionyl chloride and stirred at room temperature for 14 h. After removing excess thionyl chloride, the crude acid chloride was mixed with a solution of 2-(6-phenylhexyl)thiophene in dichloromethane (DCM) and cooled to 0^o^C; anhydrous tin chloride was then slowly added to it. After purification, the product was chromatographed on silica gel to obtain a crude product (i.e., a keto ester) with a yield of 83%.

The keto ester was suspended in diethylene glycol containing potassium hydroxide and hydrazine hydrate. The mixture was distilled until the temperature reached 200°C, and then it was refluxed for 3 h. The mixture was then cooled to 90°C, poured into water, and acidified to a pH between 2 and 3 with 12-N HCl. The acidified mixture was then extracted thoroughly with ether, washed with water, and dried over anhydrous sodium sulfate to obtain 2-(3-(R,S)-methyl-4-carboxybutyl)-5-(6-phenylhexyl)-thiophene, an acid. The yield of this reaction was 90%.

A Raney nickel suspension was added to the thiophene product and mixed with ethanol and sodium carbonate. The mixture was stirred vigorously under reflux for 16 h and filtered. The filtrate was cooled, acidified, and extracted with ether. The ether extract was washed four times with water and dried over anhydrous sodium sulfate, and the solvent was removed under vacuum to obtain 15-phenyl-3-(R,S)-methylpentadecanoic acid. The acid was chromatographed on silicic acid, and the appropriate fractions were dried under vacuum to obtain a white solid with a yield of 67%. The methyl ester was prepared using diazomethane. After purification on a silicic acid column, the methyl ester was dissolved in trifluoroacetic acid with thallium trifluoroacetate. This mixture was stirred in the dark at room temperature for 48 h, and an intermediate compound obtained after distillation was mixed with a solution of DCM containing isoamyl nitrate under red light. A solution of 12 N HCl and glacial acetic acid was added, and the mixture was stirred for 10 min. To this mixture, 1 N HCl was added, and the mixture was stirred for another 10 min and filtered through Celite to obtain a green-colored DCM layer. This extract was washed several times with 0.1 N HCl and water and dried over sodium sulfate. A green-colored oil, left behind after the solvent was evaporated under vacuum, was chromatographed on silicic acid, and a nitroso intermediate, methyl 15-(p-nitrosophenyl)-3-(R,S)-methyl-pentadecanoate, was obtained with a yield of 48% that was determined to be a single component by thin-layer chromatography (TLC).

A suspension of the nitroso intermediate was prepared in methanol containing palladium on charcoal, and it was stirred under argon at room temperature and followed by the addition of sodium borohydride in methanol. A chloroform extract was washed with water and dried over anhydrous sodium sulfate to obtain an amine, methyl 15-(p-aminophenyl)-3(R,S)-methyl-pentadecanoate, which was an orange-colored oil, after the evaporation of chloroform. The amine was purified on a silica gel column as a yellow oil with a yield of 90%.

The amine from above was suspended in 0.5 N HCl, and the mixture was cooled to 0–5^o^C, followed by the addition of a sodium nitrite solution and 5 min of stirring. Subsequently, piperidine was added to the reaction mixture over 20 min while the temperature was maintained, and the mixture was poured into water, extracted with chloroform, washed with water, dried over anhydrous sodium sulfate, and evaporated under vacuum to obtain a crude triazine, 1-[4-(13(R,S)-methyl-14-carbomethoxytetradecyl)-phenyl]3,3-(1,5-pentanediyl)triazine. This crude triazine was chromatographed on silica gel to obtain a yellow oil with a yield of 62%.

The above compound was refluxed in ethanol containing NaOH for 60 min, cooled, poured into water, and acidified to pH 3 with 1 N HCl. The mixture was extracted with ethyl ether, and the extract was washed with water. It was then dried over anhydrous sodium sulfate, and the solvent was removed to obtain a tan solid that was recrystallized from methanol-water as a light solid powder, 1-[4-(13(R,S)-methyl-14-carboxytetradecyl)-phenyl]3,3-(1,5-pentanediyl)triazine. The yield of this reaction was 53%.

This light solid powder was dissolved in acetone and added dropwise with stirring to a mixture of trifluoroacetic acid and sodium iodide at 0–5^o^C. An ethanol extract was washed with sodium sulphite and dried over anhydrous sodium sulfate. The solvent was removed under vacuum, and the resulting product, BMIPP (yield 65%), was crystallized from petroleum ether.

An alternate method for the synthesis of BMIPP and labeling with radioactive iodine (^131^I) was also described elsewhere (17).

Radioiodination of BMIPP with iodine (^123^I) was described by Sloof et al. (18) and performed with the use of the copper-assisted nucleophilic exchange method of Mertens et al. (19). Purification of [^123^I]-BMIPP was performed with a Sep-Pak RP-18 Light cartridge. Purified [^123^I]-BMIPP in ethanol was formulated in 5% human serum albumin, and the final solution was sterilized by filtration. Purity of [^123^I]-BMIPP was determined with high-performance liquid chromatography (HPLC). Radiochemical purity of [^123^I]-BMIPP was determined to be >99% with a specific activity of 5.14–5.7 mCi/μmol (190–210 MBq/μmol). The radiochemical yield and stability of the formulated product was not provided by the investigators (18).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+BMIPP+in+vitro)]

Yamamichi et al. studied the metabolism of BMIPP in isolated rat hearts (20). The rat hearts were initially perfused with HEPES buffer containing various energy substrates in bovine serum albumin (BSA), and this was followed by recirculation of the buffer for 4 h after a bolus injection of [^123^I]-BMIPP. The various metabolites in the buffer were subsequently analyzed with HPLC and TLC. More than eight BMIPP metabolites were identified when oleate served as the energy substrate, and the metabolites changed with the type of energy substrate (oleate, glucose + insulin, acetate, or BMIPP alone) in the buffer. This study showed that the metabolism of [^123^I]-BMIPP in the myocardium was closely related to the carbohydrate metabolic activity in the tissue (20).

Kropp et al studied the metabolism of [^123^I]-BMIPP in rat hearts perfused with Krebs-Henseleit buffer (pH 7.4) either with or without BSA or palmitate (21). The radioactive metabolites were determined with HPLCA and TLC analyses, and the primary metabolites of BMIPP were further characterized by electrospray mass spectrometry. The major metabolite of [^123^I]-BMIPP in the perfusion buffer was identified to be 2-(p-iodophenyl)acetic acid, and the addition of BSA or palmitate to the perfusion buffer reduced the uptake and metabolism of BMIPP. The rat heart tissue was found to contain α-methyl-14-(p-iodophenyl)tetradecanoic acid, 12-(p-iodophenyl)-substituted-dodecanoic acid, -hexanoic acid, and IPC2, in addition to [^123^I]-BMIPP. From these results the investigators concluded that [^123^I]-BMIPP was metabolized through the α- and subsequently through the β-oxidation pathways in these animals (21).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+BMIPP+rodentia)]

Myocardial perfusion and fatty acid metabolism was determined with the use of SPECT imaging with thallium-201 (^201^Tl) and [^123^I]-BMIPP to investigate the effect of exercise on the left ventricle (LV) metabolic and functional recovery in rats with myocardial transient ischemia (22). A significantly lower severity score was reported (P < 0.05) with both radiochemicals after exercise in the ischemic animals; no such change was observed in the sedentary controls. Plasma levels of the free fatty acids were reported to normalize in the ischemic trained rats, but these levels remained elevated in the ischemic, sedentary, control rats. In addition, the exercised rats had a significant increase in the LV stroke volume (P < 0.05) and hypertrophy. The investigators concluded that the myocardial perfusion, fatty acid metabolism, and LV function improved in the animals as a result of exercise training after transient ischemia (22).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+BMIPP+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+BMIPP+non+human+primates)]

Dormehl et al. compared the use of ortho- and para-[^123^I]-15-(iodophenyl)pentadecanoic acid (oPPA and pPPA, respectively) and [^123^I]-BMIPP for planar myocardial imaging in baboons (23). From this study the investigators concluded that these radiochemicals could be used to study the myocardial metabolism. Among these labeled compounds, [^123^I]-BMIPP produced the best images and primarily reflected the tracer incorporation in the neutral lipids.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+BMIPP+humans)]

It is pertinent to mention that a large number of human studies that deal with myocardial imaging with [^123^I]-BMIPP are available. Because it is out of the scope of this chapter to cover all studies, only a select few recent studies are presented in this section. Interested readers are encouraged to visit the PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+BMIPP) site for an exhaustive list of studies available on [^123^I]-BMIPP imaging.

Inoue et al. used [^123^I]-BMIPP and ^201^TI myocardial scintigraphy to study cardiac events in 33 patients with dilated cardiomyopathy (24). Among these patients, 9 patients had a cardiac event (event group) whereas the other 24 patients were event-free (event-free group). Images obtained with [^123^I]-BMIPP and ^201^TI were divided into 17 segments, and the total defect score was calculated for each. Compared with ^201^TI, the total defect score was significantly higher (P < 0.05) with [^123^I]-BMIPP for individuals in the event group compared with those in the event-free group. With results from this study the investigators concluded that [^123^I]BMIPP was a good predictor of cardiac events in patients with dilated cardiomyopathy (24).

The relationship of [^123^I]-BMIPP uptake to rest myocardial blood flow (MBF), hyperemic MBF, and myocardial reserve flow (MRF) was assessed with radioactive oxygen [^15^O]-water positron emission tomography (PET) (25). For the study, 21 patients with chronic stable angina and no previous infarction were enrolled, and all underwent imaging with [^123^I]-BMIPP and [^15^O]-water. The investigators observed that, as the [^123^I]-BMIPP uptake decreased, the MBF and the MRF were also reduced. The investigators concluded that, in patients with chronic stable angina and no previous infarction, a lower [^123^I]-BMIPP uptake indicated a decreased cardiac MRF (25).

The use of a combination of tetrofosmin radiolabeled with meta-stable technetium ([^99m^Tc]-TF) and [^123^I]-BMIPP SPECT, a combination of [^18^F]-FDG PET and [^123^I]-BMIPP SPECT, or a combination of [^18^F]-FDG PET and [^99m^Tc]-TF SPECT were compared to predict functional improvement of ischemic myocardium in 10 patients <3 weeks after a large acute myocardial infarction (26). The sensitivity, specificity, and accuracy of the various combinations are shown in the table below.

Combination | Sensitivity (%) | Specificity (%) | Accuracy (%)
[^99m^Tc]-TF + [^123^I]-BMIPP | 61 | 83 | 70
[^18^F]-FDG + [^123^I]-BMIPP | 94 | 40 | 71
[^18^F]-FDG + [^99m^Tc]-TF | 76 | 49 | 63

With results obtained from this study, the investigators concluded that the use of [^99m^Tc]-TF and [^123^I]-BMIPP for SPECT was suitable to predict functional improvements of ischemic myocardium after a large acute myocardial infarction (26).

The myocardial creatine (CR) concentration and changes in cardiac fatty acid metabolism were investigated in 34 patients with different heart diseases (27). Gated 1H magnetic resonance spectroscopy, applying point-resolved spectroscopy, was used to measure the CR concentration of the septum in the patients. Of these patients, only 14 patients underwent [^123^I]-BMIPP myocardial scintigraphy to evaluate myocardial fatty acid metabolism. The heart/mediastinum count ratio was used to determine the uptake of [^123^I]-BMIPP. The myocardial CR concentration was reported to correlate positively with the LV ejection fraction by echocardiography (R = 0.61, P < 0.001) for all of the patients. A similar correlation was observed between [^123^I]-BMIPP uptake and LV ejection fraction (R = 0.60, P < 0.05 for initial imaging; R = 0.63, P < 0.05 for delayed imaging). The investigators concluded that there was an association between CR depletion and reduced fatty acid metabolism in patients with cardiac disease (27).

## Supplemental Information

[Disclaimers]

## References

1 Taki J. Matsunari I. Metabolic imaging using SPECT Eur J Nucl Med Mol Imaging 2007 34Suppl 1S34 48 17479263
2 Liedtke A.J. (1981). Alterations of carbohydrate and lipid metabolism in the acutely ischemic heart. Prog Cardiovasc Dis.
3 Sloof G.W., Visser F.C., van Lingen A., Bax J.J., Eersels J., Teule G.J., Knapp F.F. (1997). Evaluation of heart-to-organ ratios of 123I-BMIPP and the dimethyl-substituted 123I-DMIPP fatty acid analogue in humans. Nucl Med Commun.
4 Brinkmann J.F., Abumrad N.A., Ibrahimi A., van der Vusse G.J., Glatz J.F. (2002). New insights into long-chain fatty acid uptake by heart muscle: a crucial role for fatty acid translocase/CD36. Biochem J.
5 Ambrose K.R., Owen B.A., Goodman M.M., Knapp F.F. (1987). Evaluation of the metabolism in rat hearts of two new radioiodinated 3-methyl-branched fatty acid myocardial imaging agents. Eur J Nucl Med.
6 Mokler F.T., Lin Q., Luo H., McPherson D.W., Beets A.L., Bockisch A., Kropp J., Knapp F.F. (1999). Dual-label studies with [125I]-3(R)/[131I]-3(S)-BMIPP show similar metabolism in rat tissues. J Nucl Med.
7 Lin Q., Luo H., Mokler F., Beets A.L., Ambrose K.R., McPherson D.W., Kropp J., Knapp F.F. (1997). Effects of configuration on the myocardial uptake of radioiodinated 3(R)-BMIPP and 3(S)-BMIPP in rats. J Nucl Med.
8 Morishita S., Kusuoka H., Yamamichi Y., Suzuki N., Kurami M., Nishimura T. (1996). Kinetics of radioiodinated species in subcellular fractions from rat hearts following administration of iodine-123-labelled 15-(p-iodophenyl)-3-(R,S)-methylpentadecanoic acid (123I-BMIPP). Eur J Nucl Med.
9 Shinmura K., Tani M., Suganuma Y., Hasegawa H., Hayashi Y., Guo X.D., Nakamura Y. (1998). Myocardial uptake of iodine-125-labeled 15-(p-iodophenyl)-3-(R,S)-methyl pentadecanoic acid is decreased in chronic diabetic rats with changes in subcellular distribution. Jpn Circ J.
10 Pastore C.J. Babich J.W. Udelson J.E. Future directions of myocardial fatty acid imaging J Nucl Cardiol 2007 14Suppl3 S153 63 17556184
11 Akashi Y.J., Kida K., Suzuki K., Inoue K., Kawasaki K., Yamauchi M., Musha H., Anker S.D. (2007). The significance of 123I-BMIPP delayed scintigraphic imaging in cardiac patients. Int J Cardiol.
12 Nishimura M., Hashimoto T., Kobayashi H., Fukuda T., Okino K., Yamamoto N., Fujita H., Inoue Tsunehiko Nishimura N., Ono T. (2004). Myocardial scintigraphy using a fatty acid analogue detects coronary artery disease in hemodialysis patients. Kidney Int.
13 Nishimura M., Tsukamoto K., Hasebe N., Tamaki N., Kikuchi K., Ono T. (2008). Prediction of cardiac death in hemodialysis patients by myocardial fatty acid imaging. J Am Coll Cardiol.
14 Nishimura M., Murase M., Hashimoto T., Kobayashi H., Yamazaki S., Imai R., Okino K., Fujita H., Inoue N., Takahashi H., Ono T. (2006). Influence of diabetes mellitus on diagnostic potential of iodine-123-BMIPP imaging for coronary artery stenosis in hemodialysis patients. J Nephrol.
15 Elmalch, D.R., Stereoisomers of fatty acid analogs for diagnostic imaging., U.S.P. Office, Editor. 2008, Molecular Insight Pharmaceuticals, Inc.: United States of America.
16 Goodmen M.M., Knapp F.F., Elmaleh D.R., Strauss H.W. (1984). New myocardial imaging agents: Synthesis of 15-(p-[123I]iodophenyl)-3(R,S)-methylpentadecanoic acid by decomposition of a 3,3-(1,5-pentanedyl)triazene precursor. J. Org. Chem.
17 Goodman M.M., Kirsch G., Knapp F.F. (1984). Synthesis and evaluation of radioiodinated terminal p-iodophenyl-substituted alpha- and beta-methyl-branched fatty acids. J Med Chem.
18 Sloof G.W., Visser F.C., Bax J.J., van Lingen A., Eersels J., Knapp F.F., Teule G.J. (1998). Increased uptake of iodine-123-BMIPP in chronic ischemic heart disease: comparison with fluorine-18-FDG SPECT. J Nucl Med.
19 Mertens J., Vanryckeghem W., Gysemans M., Eersels J., Finda-Panek E., Carlsen L. (1987). New fast preparation of 123I labelled radiopharmaceuticals. Eur J Nucl Med.
20 Yamamichi Y., Kusuoka H., Morishita K., Shirakami Y., Kurami M., Okano K., Itoh O., Nishimura T. (1995). Metabolism of iodine-123-BMIPP in perfused rat hearts. J Nucl Med.
21 Kropp J., Eisenhut M., Ambrose K.R., Knapp F.F., Franke W.G. (1999). Pharmacokinetics and metabolism of the methyl-branched fatty acid (BMIPP) in animals and humans. J Nucl Med.
22 Chen L., Nohara R., Hirai T., Li X., Kataoka K., Hosokawa R., Masuda D., Fujita M., Taguchi S., Sasayama S. (2001). Effects of exercise training on myocardial fatty acid metabolism in rats with depressed cardiac function induced by transient ischemia. Jpn Circ J.
23 Dormehl I.C., Hugo N., Rossouw D., White A., Feinendegen L.E. (1995). Planar myocardial imaging in the baboon model with iodine-123-15-(iodophenyl)pentadecanoic acid (IPPA) and iodine-123-15-(P-iodophenyl)-3-R,S-methylpentadecanoic acid (BMIPP), using time-activity curves for evaluation of metabolism. Nucl Med Biol.
24 Inoue A., Fujimoto S., Yamashina S., Yamazaki J. (2007). Prediction of cardiac events in patients with dilated cardiomyopathy using 123I-BMIPP and 201Tl myocardial scintigraphy. Ann Nucl Med.
25 Kageyama H., Morita K., Katoh C., Tsukamoto T., Noriyasu K., Mabuchi M., Naya M., Kawai Y., Tamaki N. (2006). Reduced 123I-BMIPP uptake implies decreased myocardial flow reserve in patients with chronic stable angina. Eur J Nucl Med Mol Imaging.
26 Seki H., Toyama T., Higuchi K., Kasama S., Ueda T., Seki R., Hatori T., Endo K., Kurabayashi M. (2005). Prediction of functional improvement of ischemic myocardium with (123I-BMIPP SPECT and 99mTc-tetrofosmin SPECT imaging: a study of patients with large acute myocardial infarction and receiving revascularization therapy. Circ J.
27 Nakae I., Mitsunami K., Matsuo S., Horie M. (2007). Creatine depletion and altered fatty acid metabolism in diseased human hearts: clinical investigation using 1H magnetic resonance spectroscopy and 123I BMIPP myocardial scintigraphy. Acta Radiol.